# N-(3-Fluoropropyl)-2β-carbomethoxy-3β-(4-[^123^I]iodophenyl)nortropane

Chemical name: | N-(3-Fluoropropyl)-2β-carbomethoxy-3β-(4-[^123^I]iodophenyl)nortropane
Abbreviated name: | [^123^I]FP-CIT, [^123^I]β-CIT-FP
Synonym: | 2-Carbomethoxy-8-(3-fluoropropyl)-3-(4-[^123^I]iodophenyl)tropane, N-ω-Fluoropropyl-2β-carbomethoxy-3β-(4-[^123^I]iodophenyl)tropane, 123I-Ioflupane, DaTSCAN®
Agent category: | Compound
Target: | Dopamine transporter (DAT)
Target category: | Transporter
Method of detection: | Single photon emission computed tomography (SPECT)
Source of signal: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents; - Non-Human Primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%5BAll%20Fields%5D%20AND%20%222-carbomethoxy-8-%283-fluoropropyl%29-3-%284-iodophenyl%29tropane%22%5BSubstance%20Name%5D)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition and emotion. Parkinson’s disease (PD) is associated with a loss of dopamine-containing neurons in striatum, resulting in a loss of dopamine transporters (DAT) in the presynaptic nerve terminals (1, 2). Reduction of DAT density is inversely correlated with the severity of motor dysfunction in PD patients. Several cocaine analogs were developed for the evaluation of DAT density in neurons of PD patients. Radiolabeled 2β-carboxymethoxy-3β-(4-iodophenyl)tropane (β-CIT) and N-(3-fluoropropyl)-2β-carbomethoxy-3β-(4-iodophenyl)nortropane (FP-CIT) have been used for brain imaging (3-6). Because of the short physical half-live of [^11^C] of [^11^C]-analogues, equilibrium conditions are difficult to achieve in positron emission tomography (PET) measurements. [^123^I]β-CIT was studied in single photon emission computed tomography (SPECT), showing slow tracer uptake kinetics (7, 8). It took 20 to 30 h to reach a stable level in the striatum. Therefore, [^123^I]FP-CIT was developed for SPECT brain imaging in PD patients (4). [^123^I]FP-CIT was approved by the United States Food and Drug Administration (FDA) for detecting loss of functional nigrostriatal dopaminergic neurons by SPECT imaging in patients presenting with symptoms or signs suggestive of dopaminergic neurodegeneration in 2011.

### Related Resource Links:

- Chapters in MICAD (Dopamine transporter (http://www.ncbi.nlm.nih.gov/books?term=dopamine%20transporter%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Dopamine transporter (http://www.ncbi.nlm.nih.gov/gene/6531))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Dopamine transporter (http://www.ncbi.nlm.nih.gov/omim/126455))
- Clinical trials ([^123^I]FP-CIT (http://www.clinicaltrials.gov/ct2/results?term=DatSCAN))
- Drug information in FDA ([^123^I]FP-CIT (http://google2.fda.gov/search?q=DatSCAN&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=19&y=6))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%5BAll%20Fields%5D%20AND%20%222-carbomethoxy-8-%283-fluoropropyl%29-3-%284-iodophenyl%29tropane%22%5BSubstance%20Name%5D%20AND%20synthesis)]

[^123^I]FP-CIT was synthesized by the chloramine-T method to iodinate the trimethylstannyl precursor using sodium [^123^I]iodide. This method gave a radiochemical yield of 95% and a radiochemical purity of 98% (4). [^123^I]FP-CIT is also commercially available (Amersham, Cygne, The Netherlands).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%5BAll%20Fields%5D%20AND%20%222-carbomethoxy-8-%283-fluoropropyl%29-3-%284-iodophenyl%29tropane%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

FP-CIT was reported to bind to both dopaminergic and serotonergic transporters in rat forebrain membrane homogenates (9). The transporter-binding affinity of FP-CIT was evaluated by competitive radioaffinity assays for DAT, serotonin, and norepinephrine with [^3^H]GBR 12935, [^3^H]paroxetine, and [^3^H]nisoxetine, respectively. Binding affinity (K_i_, nM) of FP-CIT at DAT, serotonin, and norepinephrine were 3.50, 0.11, and 63.0, respectively. FP-CIT showed lower DAT affinity than β-CIT for DAT and was more selective for serotonin over DAT. Therefore, [^123^I]FP-CIT is useful as a tracer for DA neurons in the striatum and for serotonin neurons in the other brain areas.

## Animal Studies

### Rodent Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%5BAll%20Fields%5D%20AND%20%222-carbomethoxy-8-%283-fluoropropyl%29-3-%284-iodophenyl%29tropane%22%5BSubstance%20Name%5D%20AND%20rodentia)]

Intravenous injection of [^123^I]FP-CIT in rats resulted in high uptake of radioactivity in the striatum (10). Less pronounced uptake was seen in hypothalamus areas with high serotonin uptake sites. The striatal uptake of [^123^I]FP-CIT was displaced significantly by GBR 12,909 (a specific DAT blocker) and not by fluvoxamine (a specific serotonin re-uptake blockers). On the other hand, fluvoxamine decreased [^123^I]FP-CIT accumulation in the hypothalamus. The other organs with significant uptake were the liver, spleen, kidneys, and lung. Neither GBR 12,909 nor fluvoxamine blocked the uptake in these organs. In another study, Lavalaye et al. (11) showed that acute and sub-chronic administration of various dopaminergic drugs did not have any effect on [^123^I]FP-CIT uptake in the striatum.

### Other Non-Primate Mammal Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%5BAll%20Fields%5D%20AND%20%222-carbomethoxy-8-%283-fluoropropyl%29-3-%284-iodophenyl%29tropane%22%5BSubstance%20Name%5D%20AND%20%28dog%20or%20pig%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primate Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28123I%5BAll%20Fields%5D%20AND%20%222-carbomethoxy-8-%283-fluoropropyl%29-3-%284-iodophenyl%29tropane%22%5BSubstance%20Name%5D%29%20AND%20monkeys%5BText%20Word%5D)]

SPECT studies were performed in baboons with [^123^I]FP-CIT (12). The tracer entered the brain rapidly. There was a high uptake in the striatum and much lower uptake in the midbrain, occipital cortex, and cerebellum. The striatum/cerebellum ratio was about 3-4 at the time of peak uptake (30-60 min) and increased to 6-10 after 5 h. [^123^I]FP-CIT kinetics were slow, with specific striatal washout rates of 5-7%/h, and showed major accumulation in the urinary bladder intestines, liver, kidneys and brain.

Monkeys were unilaterally treated with neurotoxic doses of 1-methyl-4-phenyl-1,2,3,6-tetrahydropyridine (MPTP) (10). There was a severe loss of striatal uptake of [^123^I]FP-CIT at the treated side as compared with the untreated side. The striatum/cerebellum ratio was 3.9 at 3 h in the control monkeys. The ratio was 1 in the MPTP-lesioned monkeys.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%5BAll%20Fields%5D%20AND%20%222-carbomethoxy-8-%283-fluoropropyl%29-3-%284-iodophenyl%29tropane%22%5BSubstance%20Name%5D%20AND%20human)]

Human dosimetry of [^123^I]FP-CIT was determined from blood samples and SPECT images in 12 human subjects after intravenous injection of 100 MBq (2.7 mCi) of [^123^I]FP-CIT, which was cleared rapidly from the blood to 53% in 60 min (13). High uptake in the lungs and liver was observed after 10 min, with lower radioactivity in the brain and intestines. The images at 24 and 48 h showed persistent uptake in the liver, lungs, striatum, intestines, and urinary bladder. The effective dose equivalent was estimated to be 0.024 mSv/MBq (2.4 rem/mCi). The organ that received the highest dose was the striatum (0.23 mGy/MBq (0.85 rad/mCi)), followed by the urinary bladder (0.054 mGy/MBq (0.20 rad/mCi)), lungs (0.043 mGy/MBq (0.16 rad/mCi)), and liver (0.029 mGy/MBq (0.11 rad/mCi)).

It was reported that there is a significant correlation of PD severity and duration with [^123^I]FP-CIT SPECT striatal uptake (14-16). In a recent study with 30 patents, [^123^I]FP-CIT brain scans were compared with magnetic resonance imaging (MRI)/computed tomography (CT) scans (17). In 5 patients with normal [^123^I]FP-CIT brain SPECT and MRI/CT scans, symptoms could be related to a benign disorder, such as essential tremor. Two patients had non-diagnostic FP-CIT brain SPECT, with MRI/CT scans compatible with subcortical cerebrovascular disease. In the remaining 23 patients, abnormal striatal [^123^I]FP-CIT uptake correlated with neurological findings, significantly increasing the probability of PD. In these patients, MRI/CT scans were normal or showed mild brain atrophy or cerebral vascular disease. [^123^I]FP-CIT scan is a useful tool in clinical practice to support the diagnosis of PD and to differentiate among other conditions [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%5BAll%20Fields%5D%20AND%20%222-carbomethoxy-8-%283-fluoropropyl%29-3-%284-iodophenyl%29tropane%22%5BSubstance%20Name%5D%20AND%20human)]. Moreover, [^123^I]FP-CIT SPECT could significantly affect treatment selection and be used to noninvasively monitor the effectiveness of the therapies of these patients.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Abi-Dargham A., Gandelman M.S., DeErausquin G.A., Zea-Ponce Y., Zoghbi S.S., Baldwin R.M., Laruelle M., Charney D.S., Hoffer P.B., Neumeyer J.L., Innis R.B. (1996). SPECT imaging of dopamine transporters in human brain with iodine-123-fluoroalkyl analogs of beta-CIT. J Nucl Med.
4 Chaly T., Dhawan V., Kazumata K., Antonini A., Margouleff C., Dahl J.R., Belakhlef A., Margouleff D., Yee A., Wang S., Tamagnan G., Neumeyer J.L., Eidelberg D. (1996). Radiosynthesis of [18F] N-3-fluoropropyl-2-beta-carbomethoxy-3-beta-(4-iodophenyl) nortropane and the first human study with positron emission tomography. Nucl Med Biol.
5 Kazumata K., Dhawan V., Chaly T., Antonini A., Margouleff C., Belakhlef A., Neumeyer J., Eidelberg D. (1998). Dopamine transporter imaging with fluorine-18-FPCIT and PET. J Nucl Med.
6 Lundkvist C., Halldin C., Ginovart N., Swahn C.G., Farde L. (1997). [18F] beta-CIT-FP is superior to [11C] beta-CIT-FP for quantitation of the dopamine transporter. Nucl Med Biol.
7 Ishikawa T., Dhawan V., Kazumata K., Chaly T., Mandel F., Neumeyer J., Margouleff C., Babchyck B., Zanzi I., Eidelberg D. (1996). Comparative nigrostriatal dopaminergic imaging with iodine-123-beta CIT-FP/SPECT and fluorine-18-FDOPA/PET. J Nucl Med.
8 Laruelle M., Wallace E., Seibyl J.P., Baldwin R.M., Zea-Ponce Y., Zoghbi S.S., Neumeyer J.L., Charney D.S., Hoffer P.B., Innis R.B. (1994). Graphical, kinetic, and equilibrium analyses of in vivo [123I] beta-CIT binding to dopamine transporters in healthy human subjects. J Cereb Blood Flow Metab.
9 Neumeyer J.L., Tamagnan G., Wang S., Gao Y., Milius R.A., Kula N.S., Baldessarini R.J. (1996). N-substituted analogs of 2 beta-carbomethoxy-3 beta- (4'-iodophenyl)tropane (beta-CIT) with selective affinity to dopamine or serotonin transporters in rat forebrain. J Med Chem.
10 Booij J., Andringa G., Rijks L.J., Vermeulen R.J., De Bruin K., Boer G.J., Janssen A.G., Van Royen E.A. (1997). [123I]FP-CIT binds to the dopamine transporter as assessed by biodistribution studies in rats and SPECT studies in MPTP-lesioned monkeys. Synapse.
11 Lavalaye J., Knol R.J., de Bruin K., Reneman L., Janssen A.G., Booij J. (2000). [123I]FP-CIT binding in rat brain after acute and sub-chronic administration of dopaminergic medication. Eur J Nucl Med.
12 Baldwin R.M., Zea-Ponce Y., al-Tikriti M.S., Zoghbi S.S., Seibyl J.P., Charney D.S., Hoffer P.B., Wang S., Milius R.A., Neumeyer J.L., et al. (1995). Regional brain uptake and pharmacokinetics of [123I]N-omega-fluoroalkyl-2 beta-carboxy-3 beta-(4-iodophenyl)nortropane esters in baboons. Nucl Med Biol.
13 Booij J., Busemann Sokole E., Stabin M.G., Janssen A.G., de Bruin K., van Royen E.A. (1998). Human biodistribution and dosimetry of [123I]FP-CIT: a potent radioligand for imaging of dopamine transporters. Eur J Nucl Med.
14 Benamer H.T., Patterson J., Wyper D.J., Hadley D.M., Macphee G.J., Grosset D.G. (2000). Correlation of Parkinson's disease severity and duration with 123I-FP-CIT SPECT striatal uptake. Mov Disord.
15 Booij J., Habraken J.B., Bergmans P., Tissingh G., Winogrodzka A., Wolters E.C., Janssen A.G., Stoof J.C., van Royen E.A. (1998). Imaging of dopamine transporters with iodine-123-FP-CIT SPECT in healthy controls and patients with Parkinson's disease. J Nucl Med.
16 Seibyl J.P., Marek K.L., Quinlan D., Sheff K., Zoghbi S., Zea-Ponce Y., Baldwin R.M., Fussell B., Smith E.O., Charney D.S., et al. (1995). Decreased single-photon emission computed tomographic [123I]beta-CIT striatal uptake correlates with symptom severity in Parkinson's disease. Ann Neurol.
17 Covelli E.M., Brunetti A., Di Lauro A., Sullo P., Mazzarella G., Tedeschi E., Belfiore G. (2004). Clinical impact of correlative [123I]-FP-CIT brain imaging and neurological findings in suspect Parkinson's disease. Radiol Med (Torino).